# ^99m^Tc-succinimidyl-6-hydrazinopyridine-3-carboxylate-interleukin 12

Chemical name: | ^99m^Tc-succinimidyl-6-hydrazinopyridine-3-carboxylate-interleukin 12
Abbreviated name: | ^99m^Tc-IL-12
Synonym: | ^99m^Tc-labeled IL-12
Agent Category: | IL-12
Target: | IL-12 receptor
Target Category: | Receptor-ligand binding
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the nucleotide (Alpha (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=5923852) and Beta (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=5923854) subunits) and protein precursor (Alpha (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=20141534) and Beta (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=266320) subunits) sequence of IL-12.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+IL-12)]

Interleukin 12 (IL-12) is a 75-kDa, heterodimeric, glycosylated protein that is a key cytokine for the differentiation of T helper 1 (Th1) cells, and it is also involved in the activation of natural killer (NK) cells (1). Although IL-12 is secreted mainly by monocytes, B cells, and cells positive for major histocompatibility complex II, the IL-12 receptor is expressed only on the activated T or NK cells (2). The Th1 cells are characterized by the production of interferon-γ and are believed to have a role in the development of chronic inflammatory disorders because of their function of clearing intracellular pathogens (3). Currently only a few non-invasive techniques are available for the diagnosis or monitoring of chronic inflammation and infection. Radioactive fluorine-labeled fluorodeoxyglucose (^18^F-FDG) has been used with positron emission tomography (PET) to study chronic inflammation, but it lacks specificity to distinguish inflammation from infection because of its cellular uptake mechanism (4-6). The labeling of lymphocytes with radioactive metastable technetium (^99m^Tc)-labeled hexamethyl propyleneamine oxime to study inflammation was also attempted, but the low labeling efficiency of the cells yielded poor scintigraphic images and the investigators concluded that this was not a suitable method to investigate inflammation (7). Labeled peptides have also been used to detect inflammation, but these radiopharmaceuticals did not always give optimal results and have not found much clinical application (8). Interleukin-2 (IL-2) radiolabeled with radioactive iodine (^123^I) or ^99m^Tc has been used successfully for the in vivo detection of chronic inflammation, but it was reported to be tedious and expensive to label this cytokine because it has a low solubility and stability (9, 10). Because IL-12 binds to cells that mediate inflammation, Annovazzi et al. decided to label recombinant human IL-12 (rhIL-12) with ^99m^Tc to obtain ^99m^Tc-IL-12 and evaluated the labeled cytokine to detect inflammation in a mouse model (11). Non-radioactive rhIL-12 is approved by the United States Food and Drug Administration for use in clinical trials (http://clinicaltrials.gov/ct/search?term=interleukin-12&submit=Search&interleukin.ID=term&interleukin.badWord=interlukin&interleukine.ID=term&interleukine.badWord=interlukin&interleukins.ID=term&interleukins.badWord=interlukin&interluekin.ID=term&interluek) to treat a variety of conditions.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+IL+12+synthesis)]

Details for expression and purification of the rhIL-12 used to produce ^99m^Tc-IL-12 are given elsewhere (12). Briefly, the recombinant protein was produced from the culture supernatant of mammalian cells using an appropriate expression vector. The protein was purified by a multi-step purification procedure as described by Leonard et al. (12). The cytokine has also been produced as a freeze-dried preparation (13). A previously frozen solution of IL-12 was used for the preparation of ^99m^Tc-IL-12 (11).

Succinimidyl-6-hydrazinopyridine-3-carboxylate (HYNIC-NHS) was synthesized and conjugated to IL-12 using the modified method of Abrams et al. (14). The conjugated IL-12 was generated by mixing IL-12 with HYNIC-NHS dissolved in dimethyl sulphoxide at a molar ratio of 6:1 HYNIC-NHS:IL-12 for 2 h (11). An average of 1.9 mol HYNIC-NHS was conjugated to IL-12. Free HYNIC-NHS was subsequently removed from HYNIC-IL-12 on a G50 microspin column. The purity of HYNIC-IL-12 was checked by high-performance liquid chromatography (HPLC) with a size-exclusion column. Aliquots of HYNIC-IL-12 were stored at –20^o^ C until required.

The radiolabeling of HYNIC-IL-12 with ^99m^Tc to generate ^99m^Tc-IL-12 was performed in acetate buffer (pH 5.5) (11). The conjugate was incubated with ^99m^Tc for 30 min in presence of stannous chloride. The labeling efficiency was determined by instant thin-layer chromatography, and the unbound ^99m^Tc was separated from the radiolabeled compound on a microspin G50 column. The ^99m^Tc-IL-12 was analyzed by size-exclusion chromatography on HPLC (11). The labeling efficiency was determined to be between 75% and 85%, with a maximum specific activity of ~70.3 MBq/1.33 pmol (1.9 mCi/1.33 pmol). The radiochemical purity of the labeled conjugate was >95% and colloidal content was <5% in all preparations. Stability studies indicated that the labeled IL-12 lost only ~10% purity at 6 h when stored in either serum or saline (11).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+IL+12+in+vitro)]

The receptor binding of ^99m^Tc-IL-12 was investigated with Kit225 (http://www.copewithcytokines.de/cope.cgi?key=Kit225) cells (a human IL-2–dependent cell line) that constitutively express the IL-12 receptor (15). Increasing concentrations of ^99m^Tc-IL-12 were incubated with the cells at 4°C for 60 min. The cells were then harvested by centrifugation and counted for bound radioactivity (11). The mean affinity constant (K_d_) of ^99m^Tc-IL-12 was determined to be 2.09 × 10^–9^ M (P < 0.05).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+IL+12+rodentia)]

The biodistribution of ^99m^Tc-IL-12 was studied in normal mice (11). The labeled conjugate was detected primarily in the liver with significant uptake in the spleen and thymus up to 6 h after injection. The investigators suggest that the accumulation of ^99m^Tc-IL-12 in these organs was probably the result of the presence of resident T lymphocytes.

The specificity and targeting of ^99m^Tc-IL-12 was investigated in mice bearing Kit225 cell tumors (injected in a Matrigel vehicle) in the left flank. For control, mice were injected with Matrigel alone in the right flank (11). After injection of ^99m^Tc-IL-12, the mice (n = 3 per time point) were killed at different time points (1.5, 3 and 6 h) and the Matrigel pellets were removed, weighed, and counted for radioactivity. Uptake of the label was determined as percent of injected activity per gram tissue weight (% IA/g). At any given time point, the amount of radioactivity detected in the Matrigel that contained Kit225 cells was approximately twice that detected in the Matrigel alone. This indicated that the labeled IL-12 would accumulate at sites of inflammation where lymphocytes are attracted because of an immune response. No competition data with cold IL-12 was presented by the investigators (11).

The binding of ^99m^Tc-IL-12 was also investigated in mice with trinitrobenzene sulphonic acid–induced chronic colitis (11). For this study, control mice were treated with 50% ethanol in 50% phosphate buffered saline . Six mice with chronic colitis were injected with ^99m^Tc-IL-12 and killed 3 h later. The large bowel was removed, weighed, counted, and imaged with a gamma camera. The percent of secreted activity was determined by separating the stool and the intestinal wall from the inflamed tissue (11). The affected colon was divided into consecutive segments and each segment was examined histologically, weighed, and counted for radioactivity to determine uptake of the label (% IA/g). The label was observed to have accumulated primarily in the inflamed sections of the colon, and little uptake was noted in the non-inflamed sections or in the colon from the control mice. The level of label detected in the inflamed sections correlated with the degree of bowel lymphatic infiltration observed during histological evaluation. The stool was observed to contribute 10.4 ± 7.5% and 9.2 ± 3.2% of the label in affected and non-affected areas of the colon, respectively (11). Blocking studies were not reported by the investigators.

The investigators suggested that high doses of the radiochemical could be used in mice without side effects because the IL-12 receptors in these animals bind the cytokine but do not trigger biological activity (11). From these results they concluded that labeled IL-12 could potentially be used in humans only after specific activity of the radiochemical was improved and the dosage was carefully evaluated.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+IL+12+non+primate+mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+IL+12+non+human+primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+IL+12+humans)]

No publications are currently available.

## References

1 Del Vecchio M., Bajetta E., Canova S., Lotze M.T., Wesa A., Parmiani G., Anichini A. (2007). Interleukin-12: biological properties and clinical application. Clin Cancer Res.
2 Desai B.B., Quinn P.M., Wolitzky A.G., Mongini P.K., Chizzonite R., Gately M.K. (1992). IL-12 receptor. II. Distribution and regulation of receptor expression. J Immunol.
3 Harrington L.E., Hatton R.D., Mangan P.R., Turner H., Murphy T.L., Murphy K.M., Weaver C.T. (2005). Interleukin 17-producing CD4+ effector T cells develop via a lineage distinct from the T helper type 1 and 2 lineages. Nat Immunol.
4 Yamada Y., Uchida Y., Tatsumi K., Yamaguchi T., Kimura H., Kitahara H., Kuriyama T. (1998). Fluorine-18-fluorodeoxyglucose and carbon-11-methionine evaluation of lymphadenopathy in sarcoidosis. J Nucl Med.
5 Hara T., Kosaka N., Suzuki T., Kudo K., Niino H. (2003). Uptake rates of 18F-fluorodeoxyglucose and 11C-choline in lung cancer and pulmonary tuberculosis: a positron emission tomography study. Chest.
6 Ogawa M., Ishino S., Mukai T., Asano D., Teramoto N., Watabe H., Kudomi N., Shiomi M., Magata Y., Iida H., Saji H. (2004). (18)F-FDG accumulation in atherosclerotic plaques: immunohistochemical and PET imaging study. J Nucl Med.
7 Jaakkola K., Knuuti J., Soderlund K., Saraste A., Jalkanen S., Voipio-Pulkki L.M. (1998). Labelling lymphocytes with technetium99m-hexamethyl propyleneamine oxime for scintigraphy: an improved labelling procedure. J Immunol Methods.
8 Chianelli M., Parisella M.G., D'Alessandria C., Corsetti F., Scopinaro F., Signore A. (2003). The developing role of peptide radiopharmaceuticals in the study of chronic inflammation: new techniques for novel therapeutic options. Q J Nucl Med.
9 Annovazzi A., Bonanno E., Arca M., D'Alessandria C., Marcoccia A., Spagnoli L.G., Violi F., Scopinaro F., De Toma G., Signore A. (2006). 99mTc-interleukin-2 scintigraphy for the in vivo imaging of vulnerable atherosclerotic plaques. Eur J Nucl Med Mol Imaging.
10 Signore A., Picarelli A., Annovazzi A., Britton K.E., Grossman A.B., Bonanno E., Maras B., Barra D., Pozzilli P. (2003). 123I-Interleukin-2: biochemical characterization and in vivo use for imaging autoimmune diseases. Nucl Med Commun.
11 Annovazzi A., D'Alessandria C., Bonanno E., Mather S.J., Cornelissen B., van de Wiele C., Dierckx R.A., Mattei M., Palmieri G., Scopinaro F., Signore A. (2006). Synthesis of 99mTc-HYNIC-interleukin-12, a new specific radiopharmaceutical for imaging T lymphocytes. Eur J Nucl Med Mol Imaging.
12 Leonard J., Goldman S., O'Hara R. (2006).
13 Warne N.W., Crowley T.J., Smith T.M. (1998).
14 Abrams M.J., Juweid M., tenKate C.I., Schwartz D.A., Hauser M.M., Gaul F.E., Fuccello A.J., Rubin R.H., Strauss H.W., Fischman A.J. (1990). Technetium-99m-human polyclonal IgG radiolabeled via the hydrazino nicotinamide derivative for imaging focal sites of infection in rats. J Nucl Med.
15 Hori T., Uchiyama T., Tsudo M., Umadome H., Ohno H., Fukuhara S., Kita K., Uchino H. (1987). Establishment of an interleukin 2-dependent human T cell line from a patient with T cell chronic lymphocytic leukemia who is not infected with human T cell leukemia/lymphoma virus. Blood.